# [^111^In]-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-heat-stable human Escherichia coli enterotoxin

Chemical name: | [^111^In]-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-heat-stable human Escherichia coli enterotoxin
Abbreviated name: | [^111^In]DOTA-F^19^-ST_h_(1-19)
Synonym: | [^111^In]-ST_h_(1-19); enterotoxin
Agent Category: | Peptide
Target: | Guanylate cyclase receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of Signal/Contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure of DOTA-F^19^-ST_h_(1-19).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Escherichia+coli+111in+enterotoxin+)]

Colorectal cancer (CRC) is the second most common neoplastic condition detected in the men and women of the United States. In 2008 it is estimated that ~150,000 individuals will be diagnosed with this disease and that it will result in the death of nearly one third of the patients (1). Most of the patients who have this cancer die because it metastasizes to the liver, and early screening of the neoplasm would help devise a suitable and favorable treatment for the patient (2). The United States Food and Drug Administration has approved radioimmunoscintigraphic agents that are based on monoclonal antibodies for the imaging of colorectal cancers, but these agents have limitations because of incomplete penetration in tumors as a result of their large molecular size and prolonged blood circulation (3, 4). A smaller IgG1-derived Fab’ fragment derived from a murine antibody has been shown to have better tumor penetration, more rapid blood clearance, reduced accumulation in nontarget tissue, and high clinical utility because the Fab’ fragment was reported to have superior imaging properties compared to the conventional diagnostic modalities (5). This indicates that a smaller radiopharmaceutical is a superior diagnostic agent with suitable pharmacodynamic properties. In addition, it has been shown that radiolabeled peptides are extremely useful for the imaging and radiotherapy of neuroendocrine and pulmonary tumors (6, 7). Among the various labeled peptides, the Escherichia coli heat-stable enterotoxin (ST_h_) has been used to image colorectal cancers (8, 9).

The ST_h_ is known to target guanylate cyclase C (GC-C), a type I transmembrane glycoprotein that is known to be the target that was expressed on intestinal brush border membranes and the human colon cancer T-84 cell line. The glycoprotein is expressed in very low amounts on the extraintestinal tissues and is expressed primarily on the primary and metastatic colon cancer tissues, therefore making it a unique marker for colorectal cancer tumors (10). Peptides such as the ST_h_ and uroguanylin have been shown to inhibit the growth of colorectal cancer cells and are efficacious in the treatment of this cancer in animal models (11-13). The enterotoxin has been shown to behave like an agonist for the GC-C receptor, resulting in activation of the guanylyl cyclase that increased the intracellular concentrations of guanosine 3,5-cyclic monophosphate, which directly influenced the fluid and electrolyte balance in the cells (14, 15). Several studies are available in which 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) derivatives of ST_h_ have been evaluated for in vitro and in vivo activities in mice bearing xenograft tumors (8, 9, 16, 17). These studies are presented in this chapter.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of ^111^In-labeled ST_h_ was described by Giblin et al. (9). The N-hydroxysuccinimide (NHS) ester of DOTA (NHS-DOTA) and the F^19^-ST_h_(1-19) peptide were obtained from commercial sources. To prepare the DOTA conjugate of the peptide, 100-fold molar excess of NHS-DOTA was incubated with the E. coli heat-stable, folded enterotoxin at 4°C overnight in HEPES buffer (pH 8.5). A yield of the DOTA-peptide conjugate was>90%, but the number of DOTA residues bound per molecule was not reported. The conjugated peptide was then purified with high-performance liquid chromatography (HPLC) using a Phenomenex Jupiter C18 column.

To label the peptide with indium (^111^In), the radioactive metal was added as indium chloride (^111^InCl_3_) to a solution of DOTA-F^19^-ST_h_(1-19) in ammonium acetate buffer (pH 6.0), and the mixture was incubated at 80°C for 1 h (9). A 0.002 M solution of ethylendiamine tetraacetic acid was subsequently added to the mixture to stop the reaction and to remove excess ^111^InCl_3_. The labeled, no carrier added, peptide conjugates were then purified from the mixture with reverse-phase HPLC (RP-HPLC). The ^111^In-ST_h_ conjugate was then concentrated through a 3 M Empore C-18 HD high-performance extraction disk cartridge, and the volume was reduced under a stream of nitrogen. The radiochemical yield of the reaction was reported to be >90% after RP-HPLC (9). The specific activity, radiochemical purity, and stability of the labeled peptide were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+enterotoxin+in+vitro)]

Gali et al. coupled a paraisothiocyanato benzyl derivative of DOTA (DOTA-NCS) to the ST_h_ peptide for the chelation of ^111^In to produce ^111^In-DOTA-NCS-ST_h_ and evaluated its in vitro activity with T-84 and CaCO-2 cells (16). The 50% inhibitory concentration (IC_50_) of ^111^In-DOTA-NCS-ST_h_ was reported to be 1.9 ± 1.0 nM and 4.6 ± 4.0 nM, respectively, for T-84 and CaCO-2 cells compared with an IC_50_ of 2.2 ± 0.8 and 3.9 ± 2.1 nM for the two cell types with ST_h_(1-19) alone.

The in vitro binding characteristics of ^111^In-ST_h_ were studied using T-84 human colorectal cancer cells (9). Compared with F^19^-ST_h_(1-19), the DOTA-conjugated analog had a two-fold higher IC_50_: 3.9 ± 1.4 nM versus 2.2 ± 0.4 nM, respectively. After labeling with indium, the IC_50_ was reported to be 5.6 ± 1.4 nM, approximately three-fold higher than the natural peptide.

In another study, the in vitro binding characteristics of ^111^In-DOTA-F^19^-ST_h_(1-19) were compared in T-84 cells for two analogs, DOTA-R^1,4^,F^19^-ST_h_(1-19), which has arginine residues instead of asparagines at positions 1 and 4, and DOTA-11AUN-F^19^-ST_h_(1-19), which has an 11-aminoundecanoic acid spacer (AUN) between the DOTA group and the first asparagine residue of the peptide (8). Substitution of the asparagines residues at positions 1 and 4 with arginine resulted in decreased hydrophobicity, whereas inclusion of the AUN spacer gave a more hydrophobic compound (8). The IC_50_ values for the In-labeled R^1,4^- and AUN-substituted compounds were 4.1 ± 3.3 and 6.0 ± 0.7 nM, respectively, compared with 4.9 ± 2.8 for the native In-DOTA-F^19^-ST_h_(1-19) compound. In the absence of unlabeled ST_h_ analogs, 9–15% of the labeled analog was associated with the T-84 cells, but addition of the unlabeled analog resulted in <3% binding to the cells. The in vitro binding and internalization of all the analogs to the cells was reported to gradually increase during a 100-min incubation period (8).

In another study, the ST_h_ was shown to bind MDA-MB-231 and T-47D cell lines derived from human breast cancer (18). However, the peptide was shown to target an unknown receptor because these cells lack the RNA transcripts for GC-C as determined with reverse-transcriptase polymerase chain reaction using the total RNA extract of the respective cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+enterotoxin+rodentia)]

Gali et al. investigated the in vivo biodistribution of ^111^In-DOTA-NCS-ST_h_ in severe combined immune deficient (SCID) mice bearing LS-180 cell xenograft tumors; the number of animals used per time point was not reported (17). The mice were injected with the labeled peptide through the tail vein, and the animals were killed 1 h or 4 h after injection. For blocking studies an excess of non-radioactive ST_h_(1-19) was injected along with the radioactive peptide. A rapid clearance of the label from blood circulation was reported, and 1 h after injection the tumors had accumulated 0.94 ± 0.31% of injected dose/gram tissue (% ID/g). At 4 h after injection the amount of radioactivity in the tumors was reported to be 0.22 ± 0.10% ID/g. During the same period the kidneys had accumulated 15.7 ± 2.6% ID/g at 1 h and 12.0 ± 2.9% ID/g at 4 h, which indicates that the radioactivity was excreted primarily through the urinary system. Partial specificity of the peptide was demonstrated by blocking studies because a reduction of ~50% in the accumulation of radioactivity (0.46 ± 0.22% ID/g) in the tumors was observed when the labeled peptide was co-injected with the non-radioactive version of ST_h_(1-19).

The in vivo biodistribution of ^111^In-ST_h_(1-19) was investigated in SCID mice bearing human T-84 cancer cell xenograft tumors; the number of animals used per time point was not reported (9). The mice were injected with the labeled peptide through the tail vein and the animals were killed at 1, 4, and 24 h after administration of the label. The organs and tumors were removed from the animals and weighed, and accumulated radioactivity was counted. For imaging, one animal was injected with the radiochemical and single-photon emission computed tomography data were acquired 1 h later (9). A rapid clearance of ^111^In-ST_h_(1-19) from the blood was reported, and >90% of the activity was excreted through the urine at 1 h after injection. The tumor uptake at this time point was 2.35 ± 0.43% ID/g, which was higher than any other organ (the range was 0.1 ± 0.05 to 0.77 ± 0.7% ID/g) except for the kidneys, which had accumulated 3.43 ± 0.97% ID/g. At 24 h after administration, the tumor and the kidneys had 0.37 ± 0.04 and 0.93 ± 0.12% ID/g remaining in the tissue, respectively. At 4 h after injection, the tumor/blood, tumor/muscle, and tumor/kidney radioactivity ratios were 37.0, 37.0, and 0.3, respectively. By imaging uptake of the peptide was reported to be high in tumor, with some accumulation in the kidneys and a diffused retention in the intestinal tissue (9).

Giblin et al. investigated the biodistribution of ^111^In-DOTA-F^19^-ST_h_(1-19), ^111^In-DOTA-R^1,4^,F^19^-ST_h_(1-19), and ^111^In-DOTA-11AUN-F^19^-ST_h_(1-19) in SCID mice bearing T-84 cell tumors (n = 5–10 animals per analog) (8). Among these analogs the various tumor/tissue ratios were as shown in the Table below.

Ratio | Analogs
Ratio | ^111^In-DOTA-F^19^-ST_h_(1-19) | ^111^In-DOTA-R^1,4^,F^19^-ST_h_(1-19) | ^111^In-DOTA-11AUN-F^19^-ST_h_(1-19)
Tumor/blood | 5.7 | 3.7 | 4.8
Tumor/muscle | 18.1 | 20.2 | 34.7
Tumor/liver | 7.2 | 4.8 | 6.0
Tumor/kidney | 0.48 | 0.48 | 0.40

The in vivo biodistribution of ^111^In-ST_h_ was also investigated in mice bearing T-47D cell xenograft tumors (18). Blocking studies with unlabeled ST_h_ were also performed with this animal model. The investigators reported that the accumulation of the label in the breast cancer cell tumors at 1 h after injection (0.67 ± 0.23% ID/g) was significantly reduced in presence of the unlabeled peptide (0.43 ± 0.20% ID/g; P < 0.05). In these animals the label was also excreted primarily through the urinary pathway (>85%).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+enterotoxin+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+enterotoxin+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+enterotoxin+humans)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some studies presented in this chapter were supported by National Cancer Institute grant R01-CA95075 and a National Cancer Institute Center grant 1 P50 CA103130-01.

## References

1 Levin B., Lieberman D.A., McFarland B., Smith R.A., Brooks D., Andrews K.S., Dash C., Giardiello F.M., Glick S., Levin T.R., Pickhardt P., Rex D.K., Thorson A., Winawer S.J. (2008). Screening and Surveillance for the Early Detection of Colorectal Cancer and Adenomatous Polyps, 2008: A Joint Guideline from the American Cancer Society, the US Multi-Society Task Force on Colorectal Cancer, and the American College of Radiology. CA Cancer J Clin.
2 Jemal A., Siegel R., Ward E., Hao Y., Xu J., Murray T., Thun M.J. (2008). Cancer statistics, 2008. CA Cancer J Clin.
3 Goldenberg D.M., Sharkey R.M. (2007). Novel radiolabeled antibody conjugates. Oncogene.
4 Burvenich I., Schoonooghe S., Cornelissen B., Blanckaert P., Coene E., Cuvelier C., Mertens N., Slegers G. (2005). In vitro and in vivo targeting properties of iodine-123- or iodine-131-labeled monoclonal antibody 14C5 in a non-small cell lung cancer and colon carcinoma model. Clin Cancer Res.
5 Moffat F.L., Pinsky C.M., Hammershaimb L., Petrelli N.J., Patt Y.Z., Whaley F.S., Goldenberg D.M. (1996). Clinical utility of external immunoscintigraphy with the IMMU-4 technetium-99m Fab' antibody fragment in patients undergoing surgery for carcinoma of the colon and rectum: results of a pivotal, phase III trial. The Immunomedics Study Group. J Clin Oncol.
6 Antunes P., Ginj M., Zhang H., Waser B., Baum R.P., Reubi J.C., Maecke H. (2007). Are radiogallium-labelled DOTA-conjugated somatostatin analogues superior to those labelled with other radiometals?. Eur J Nucl Med Mol Imaging.
7 Tzannou I.A., Karapanagiotou E.M., Charpidou A., Dilana K., Alamara C., Christakopoulou I., Georgiou E., Syrigos K.N. (2007). The use of radiolabeled somatostatin analog scintigraphy in the staging of small cell lung cancer patients. Am J Clin Oncol.
8 Giblin M.F., Gali H., Sieckman G.L., Owen N.K., Hoffman T.J., Forte L.R., Volkert W.A. (2004). In vitro and in vivo comparison of human Escherichia coli heat-stable peptide analogues incorporating the 111In-DOTA group and distinct linker moieties. Bioconjug Chem.
9 Giblin M.F., Sieckman G.L., Watkinson L.D., Daibes-Figueroa S., Hoffman T.J., Forte L.R., Volkert W.A. (2006). Selective targeting of E. coli heat-stable enterotoxin analogs to human colon cancer cells. Anticancer Res.
10 Carrithers S.L., Barber M.T., Biswas S., Parkinson S.J., Park P.K., Goldstein S.D., Waldman S.A. (1996). Guanylyl cyclase C is a selective marker for metastatic colorectal tumors in human extraintestinal tissues. Proc Natl Acad Sci U S A.
11 Pitari G.M., Di Guglielmo M.D., Park J., Schulz S., Waldman S.A. (2001). Guanylyl cyclase C agonists regulate progression through the cell cycle of human colon carcinoma cells. Proc Natl Acad Sci U S A.
12 Pitari G.M., Zingman L.V., Hodgson D.M., Alekseev A.E., Kazerounian S., Bienengraeber M., Hajnoczky G., Terzic A., Waldman S.A. (2003). Bacterial enterotoxins are associated with resistance to colon cancer. Proc Natl Acad Sci U S A.
13 Shailubhai K., Yu H.H., Karunanandaa K., Wang J.Y., Eber S.L., Wang Y., Joo N.S., Kim H.D., Miedema B.W., Abbas S.Z., Boddupalli S.S., Currie M.G., Forte L.R. (2000). Uroguanylin treatment suppresses polyp formation in the Apc(Min/+) mouse and induces apoptosis in human colon adenocarcinoma cells via cyclic GMP. Cancer Res.
14 Krause W.J., Cullingford G.L., Freeman R.H., Eber S.L., Richardson K.C., Fok K.F., Currie M.G., Forte L.R. (1994). Distribution of heat-stable enterotoxin/guanylin receptors in the intestinal tract of man and other mammals. J Anat.
15 Hamra F.K., Eber S.L., Chin D.T., Currie M.G., Forte L.R. (1997). Regulation of intestinal uroguanylin/guanylin receptor-mediated responses by mucosal acidity. Proc Natl Acad Sci U S A.
16 Gali H., Sieckman G.L., Hoffman T.J., Kiefer G.E., Chin D.T., Forte L.R., Volkert W.A. (2001). Synthesis and in vitro evaluation of an 111In-labeled ST-peptide enterotoxin (ST) analogue for specific targeting of guanylin receptors on human colonic cancers. Anticancer Res.
17 Gali H., Sieckman G.L., Hoffman T.J., Owen N.K., Chin D.T., Forte L.R., Volkert W.A. (2001). In vivo evaluation of an 111In-labeled ST-peptide analog for specific-targeting of human colon cancers. Nucl Med Biol.
18 Giblin M.F., Gali H., Sieckman G.L., Owen N.K., Hoffman T.J., Volkert W.A., Forte L.R. (2006). In vitro and in vivo evaluation of 111In-labeled E. coli heat-stable enterotoxin analogs for specific targeting of human breast cancers. Breast Cancer Res Treat.